# 6-(2-[^18^F]Fluoroethoxy)-2-[2-(4-methylaminophenyl)ethenyl]benzoxazole

Chemical name: | 6-(2-[^18^F]Fluoroethoxy)-2-[2-(4-methylaminophenyl)ethenyl]benzoxazole
Abbreviated name: | [^18^F]BF-168
Synonym:
Agent Category: | Compound
Target: | Amyloid-β (Aβ)
Target Category: | Specific binding
Method of detection: | Positron Emission Tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5B18F%5DBF-168%29%20OR%20BF-168)]

6-(2-[^18^F]Fluoroethoxy)-2-[2-(4-methylaminophenyl)ethenyl]benzoxazole ([^18^F]BF-168) is a radioligand that was developed for positron emission tomography (PET) imaging of amyloid-β (Aβ) plaques in the central nervous system (CNS) for detection of Alzheimer’s disease (AD) (1). ^18^F is a positron emitter with a physical t_½_ of 109.7 min.

Aβ peptide was sequenced from the meningeal blood vessels of AD patients and individuals with Downs syndrome (2). Aβ peptides contain 40−42 amino acid residues and are metabolic products of Aβ precursor protein (APP) from cleavage by β and γ secretases (3). Aβ is also identified as the primary component of the neuritic plaques of AD patient brain tissue (4). Cloning of the gene that encodes the APP and its localization to chromosome 21 led to the hypothesis that Aβ accumulation is the primary event in AD pathogenesis (2, 5). This hypothesis proposes that neuronal death in AD is related to toxic effect of Aβ on the adjacent cell bodies or cell processes (6). AD is a progressive, neurogenerative disorder of the CNS that is characterized by a common set of clinical and pathological features (3). In addition to Aβ, the microtubule-associated protein tau (זּ) is also found in the cell body and axons of neurons as neurofibrillary tangles.

The search for a cure or effective treatment of AD requires in vivo detection and quantification of Aβ in the brain for efficacy evaluation of AD therapy (3). Various amyloid-imaging probes have been developed based on PET, single-photon emission computed tomography, and optical imaging. These compounds generally have high binding affinity for amyloid fibrils and adequate permeability of the blood-brain barrier (1). There is evidence that suggests substantial deposition of diffuse plaques may be the initial pathological change in AD that precedes cognitive deterioration (7). Thus, imaging agents that can detect diffuse amyloid plaques may be useful for early detection of AD. Okamura et al. (1) synthesized a series of styrylbenzoxazole derivatives that target amyloid plaques, including diffuse plaques. They found that BF-168 recognized both neuritic and diffuse plaques in vivo. [^18^F]BF-168 appeared to be a promising candidate for PET imaging of AD.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28%5B18F%5DBF-168%29%20OR%20BF-168%29%20AND%20synthesis)]

Okamura et al. (1) reported the radiosynthesis of [^18^F]BF-168. 2-(4-Methylaminophenyl)-6-(2-tosyloxyethoxy)benzoxazole obtained commercially was reacted with potassium [^18^F]fluoride and Kryptofix 222 in acetonitrile at 80ºC for 20 min. The labeled compound was purified by high-performance liquid chromatography. The radiochemical yield was 30−40%, and the radiochemical purity was >95%. The maximum specificity was 106 TBq/mmol (2,865 Ci/mmol) at the end of synthesis.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28%5B18F%5DBF-168%29%20OR%20BF-168%29%20AND%20in%20vitro)]

Okamura et al. (8) evaluated unlabeled BF-168 and several other quinoline and benzimidazole derivatives. The octanol/water (1-octanol/phosphate−buffered saline) partition coefficient of BF-168 was determined to be 62.6.

Okamura et al. (1) conducted in vitro binding assays with [^125^I]BF-168 using synthetic Aβ1-42 (diffuse plaques were exclusively positive) and Aβ1-40 for binding. The dissociation constant (K_d_) values were 6.8 ± 1.4 nM and 10.6 ± 1.5 nM for Aβ1-42 and Aβ1-40, respectively. The maximum specific binding (B_max_) values were 3.2 ± 0.55 nM and 4.1 ± 1.3 nM for Aβ1-42 and Aβ1-40, respectively. The inhibition constant (K_i_) for Aβ fibrils was determined to be 6.4 ± 1.0 nM (8). The effective concentration to achieve 50% maximal fluorescence intensity at optimal excitation wavelength (EC_50_) for Aβ fibrils was 346 ± 2.21 nM. In comparison, the EC_50_ for זּ fibrils was 1010 ± 1.72 nM.

In vitro neuropathological staining studies of unlabeled BF-168 were performed in postmortem brain tissue from four autopsy-confirmed AD cases (1). The experiments showed BF-168 clearly stained both neuritic and diffuse amyloid plaques in AD temporal brain tissue sections. BF-168 bound both Aβ1−40-positive and Aβ1−42 positive plaques. The staining and distribution patterns corresponded well to those of Aβ and זּ immunostaining in the serial sections. Little nonspecific binding of BF-168 was found in the aged normal brain sections. The results also indicated that BF-168 recognized the β-pleated sheet structure of senile plaques and neurofibrillary tangles, but not nonfibrillar forms of Aβ and זּ.

Ishikawa et al. (9) reported that BF-168 also appeared to have a high affinity for the CNS protease-resistant isoforms of prion protein (PrP) which is associated with transmissible spongiform encephalopathies. Using a cellular PrP model, the IC_50_ of BF-168 to PrP was determined to be 0.4 nM.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28%5B18F%5DBF-168%29%20OR%20BF-168%29%20AND%20rodentia)]

The in vivo binding of unlabeled BF-168 was studied in PS1/APP double transgenic mice (1). Each mouse received 4 mg/kg BF-168 by i.v. injection. Brain sections were then obtained and examined using immunostaining with anti−Aβ antibodies (6F/3D). The distribution of BF-168 corresponded well to that of both compact and diffuse Aβ. The amount of BF-168 binding appeared to reflect the density of Aβ fibrils. When the same experiment was performed in APP23 single transgenic mice with only mild depositions of amyloid plaques, BF-168 successfully detected early plaque formation in the entorhinal cortex hippocampus. No binding of BF-168 was found in the brain slices of normal wild-type mice.

In vivo brain uptake studies were done by injecting 0.240.38 MBq (6.48−10.27 μCi) of [^18^F]BF-168 into normal mice (1). Brain radioactivity levels were measured to be 3.9 ± 0.22% injected dose per gram (ID/g) at 2 min after injection. There was a good brain clearance from the normal brain slices with a clearance t_½_ of 24.7 min. The brain/blood ratio dropped from 2.0 at 10 min to 0.72 at 60 min after injection.

When [^18^F]BF-168 was injected into APP23 transgenic mice with Aβ plaques, autoradiographic images of brain sections at 180 min after injection showed high radioactivity levels in the cerebral cortex, hippocampus, and entorhinal cortex (1). The distribution closely corresponded (r = 0.923; P<0.001) with those of in vitro thioflavin-S staining. There was little nonspecific accumulation of [^18^F]BF-168 in the brain.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5B18F%5DBF-168%29%20OR%20BF-168%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5B18F%5DBF-168%29%20OR%20BF-168%29%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5B18F%5DBF-168%29%20OR%20BF-168%29%20AND%20human)]

No publication is currently available.

## References

1 Okamura N., Suemoto T., Shimadzu H., Suzuki M., Shiomitsu T., Akatsu H., Yamamoto T., Staufenbiel M., Yanai K., Arai H., Sasaki H., Kudo Y., Sawada T. (2004). Styrylbenzoxazole derivatives for in vivo imaging of amyloid plaques in the brain. J Neurosci.
2 Hardy J., Selkoe D.J. (2002). The amyloid hypothesis of Alzheimer's disease: progress and problems on the road to therapeutics. Science.
3 Wu C.Y., Pike V.W., Wang Y.M. (2005). Amyloid imaging: From benchtop to bedside. Current Topcis in Developmental Biology.
4 Masters C.L., Multhaup G., Simms G., Pottgiesser J., Martins R.N., Beyreuther K. (1985). Neuronal origin of a cerebral amyloid: neurofibrillary tangles of Alzheimer's disease contain the same protein as the amyloid of plaque cores and blood vessels. Embo J.
5 Kang J., Lemaire H.G., Unterbeck A., Salbaum J.M., Masters C.L., Grzeschik K.H., Multhaup G., Beyreuther K., Muller-Hill B. (1987). The precursor of Alzheimer's disease amyloid A4 protein resembles a cell-surface receptor. Nature.
6 Carter J., Lippa C.F. (2001). Beta-amyloid, neuronal death and Alzheimer's disease. Curr Mol Med.
7 Price J.L., Morris J.C. (1999). Tangles and plaques in nondemented aging and "preclinical" Alzheimer's disease. Ann Neurol.
8 Okamura N., Suemoto T., Furumoto S., Suzuki M., Shimadzu H., Akatsu H., Yamamoto T., Fujiwara H., Nemoto M., Maruyama M., Arai H., Yanai K., Sawada T., Kudo Y. (2005). Quinoline and benzimidazole derivatives: candidate probes for in vivo imaging of tau pathology in Alzheimer's disease. J Neurosci.
9 Ishikawa K., Kudo Y., Nishida N., Suemoto T., Sawada T., Iwaki T., Doh-Ura K. (2006). Styrylbenzoazole derivatives for imaging of prion plaques and treatment of transmissible spongiform encephalopathies. J Neurochem.